# 4-[^18^F]Fluorobenzoyl-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_

Chemical name: | 4-[^18^F]Fluorobenzoyl-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_
Abbreviated name: | 4-[^18^F]F-T140
Synonym: | 4-[^18^F]F-TN14003
Agent category: | Peptide
Target: | Chemokine receptor 4 (CXCR4)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140)]

Chemokine receptors are G-protein–coupled receptors directing cell movement toward higher concentrations of chemokines. Chemokine receptor 4 (CXCR4) and its ligand, stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and hematopoietic systems (1, 2). In addition, this CXCR4-SDF-1 receptor system has a function in the development, progression, and spread of various cancers (3), and the CXCR4 acts as a co-receptor for human immunodeficiency virus (HIV) on CD4^+^ T cells (4). It has also been suggested that CXCR4/SDF-1 interaction participates in the pathogenesis of neurodegenerative and inflammatory conditions (5). CXCR4 is expressed by many different types of cancers, and overexpression of CXCR4 in cancers indicates poor prognosis with aggressive and metastatic tumors and resistance to chemotherapy (6).

CXCR4 is considered to play an important role in HIV infections and cancers. It is critical to perform imaging studies to measure CXCR4 levels under in vivo conditions for various pathological and physiological conditions (7). ^99m^Tc-SDF-1 has been used with single-photon emission computed tomography (SPECT) to determine changes in CXCR4 expression in the heart after a myocardial infarction. ^64^Cu-1,1’-[1,4-Phenylenebis(methylene)]-bis[1,4,8,11-tetraaza-cyclotetradecane] (^64^Cu-AMD3100), an inhibitor of CXCR4 activity, has been studied with positron emission tomography (PET) (8). An ^111^In-labeled CXCR4 antagonist peptide, ^111^In-Ac-TZ14011, has been developed for SPECT imaging of CXCR4 expression in xenograft tumors in mice (9). Tamamura et al. (10) identified a 14-amino-acid peptide (T140, Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_) with high anti-HIV and CXCR4 antagonistic activities in vitro. Jacobson et al. (11) radiolabeled T140 with 4-[^18^F]fluorobenzoic acid ([^18^F]FBA) to form 4-[^18^F]fluorobenzoyl-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_ (4-[^18^F]F-T140) for PET imaging of tumor CXCR4 expression with a high tumor/background ratio.

### Related Resource Links:

- Chapters in MICAD (CXCR4 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CXCR4+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (CXCR4 (http://www.ncbi.nlm.nih.gov/gene/7852))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CXCR4 (http://www.ncbi.nlm.nih.gov/omim/162643))
- Clinical trials (CXCR4 (http://www.clinicaltrials.gov/ct2/results?term=CXCR4))
- Drug information in FDA (CXCR4 (http://google2.fda.gov/search?q=CXCR4&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20synthesis)]

Jacobson et al. (11) prepared 4-[^18^F]F-T140 with a two-step synthesis in a modular system. The T140 peptide precursor with protecting groups on both lysine residues was purchased (Pro-Immune). [^18^F]FBA was synthesized using standard nucleophilic radiofluorination ([^18^F]KF/Kryptofix 2.2.2) reaction with 50%–60% yield and >99% radiochemical purity. [^18^F]FBA and the T140 peptide with protecting groups in dimethylformamide were incubated for 40 min at room temperature, followed by hydrazine hydrolysis of the protecting groups for 10 min at room temperature. 4-[^18^F]F-T140 was purified with high-performance liquid chromatography, with a radiochemical purity of >99% and a specific activity of 7 ± 2 GBq/µmol (0.19 ± 0.05 Ci/µmol) at the end of synthesis. The overall decay-corrected yield was 15 ± 5% (n = 6). The total synthesis time was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20in%20vitro)]

Chinese hamster ovary (CHO) cells were transfected with human CXCR4 (7 × 10^5^ binding sites/cell). A receptor-binding assay was performed with ^125^I-SDF-1. 4-F-T140 exhibited 50% inhibition concentration (IC_50_) value of 2.5 nM (11). 4-F-T140 exhibited a similar IC_50_ value to inhibit Jurkat T cell migration in response to SDF-1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20rodentia)]

Jacobson et al. (11) performed ex vivo biodistribution studies of 1.9 MBq (0.050 mCi) 4-[^18^F]F-T140 in nude mice (n = 3/group) bearing the CHO and CHO-CXCR4 tumor xenografts at 1, 2, and 3 h after injection. Accumulation in the CXCR4-expressing organs increased with time. The spleen exhibited 8 ± 1% injected dose/gram (ID/g) at 1 h and 12 ± 2% ID/g at 3 h. Accumulation in bone marrow increased from 0.78 ± 0.22% ID/g at 1 h to 2.6% ± 0.65% ID/g at 3 h. The blood accumulation was unexpectedly high for a small peptide, with 14.7 ± 2.6% ID/g at 3 h. Accumulation in the liver, intestine, and kidneys was low (<5% ID/g). 4-[^18^F]F-T140 exhibited a slightly higher accumulation in the CHO-CXCR4 tumors at 1–3 h (~2.3% ID/g) than in the CXCR4-negative CHO tumors (~1.7% ID/g) at the same time point (P > 0.05). The similar accumulation in both tumors suggested that the blood flow in both tumors was similar. Co-injection of excess 4-F-T140 (10–50 µg) significantly reduced (P < 0.05) the accumulation of 4-[^18^F]F-T140 in the blood, spleen, bone marrow, and CXCR4-negative tumors at 3 h after injection, whereas the accumulation in the CHO-CXCR4 tumor was significantly increased (P < 0.05). Red blood cells were responsible for 95% of radioactivity in the blood, which was reduced to 44% by excess 4-F-T140, allowing 4-[^18^F]F-T140 to be accessible to binding to the CHO-CXCR4 tumor. The tumor/muscle and tumor/blood ratios were 2.94 ± 0.16 and 0.19 ± 0.04, respectively, at 3 h after injection of only 4-[^18^F]F-T140. Co-injection with 10 µg 4-F-T140 increased the tumor/muscle and tumor/blood ratios to 21.6 ± 7.14 and 27.05 ± 8.70, respectively. Co-injection with 50 µg 4-F-T140 produced tumor/muscle and tumor/blood ratios of 10.41 ± 5.30 and 6.15 ± 2.65, respectively.

The whole-body distribution of 4-[^18^F]F-T140 was also assessed with PET imaging at 2 h after injection in mice bearing CHO and CHO-CXCR4 tumor xenografts. Both tumors were clearly visualized along with the abdomen area. In another experiment with mice bearing only a CHO-CXCR4 tumor, co-injection of excess 4-F-T140 increased radioactivity in the tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20T140%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
7 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
8 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.
9 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
10 Tamamura H., Xu Y., Hattori T., Zhang X., Arakaki R., Kanbara K., Omagari A., Otaka A., Ibuka T., Yamamoto N., Nakashima H., Fujii N. (1998). A low-molecular-weight inhibitor against the chemokine receptor CXCR4: a strong anti-HIV peptide T140. Biochem Biophys Res Commun.
11 Jacobson O., Weiss I.D., Kiesewetter D.O., Farber J.M., Chen X. (2010). PET of tumor CXCR4 expression with 4-18F-T140. J Nucl Med.